# ^64^Cu-DOTA-Tyr^3^-c(Cys-Tyr-Trp-Lys-Thr-Cys)-Thr-Lys(cypate)-NH_2_

Chemical name: | ^64^Cu-DOTA-Tyr^3^-c(Cys-Tyr-Trp-Lys-Thr-Cys)-Thr-Lys(cypate)-NH_2_
Abbreviated name: | ^64^Cu-LS172
Synonym: | ^64^Cu-DOTA-Tyr^3^-octreotate-Lys-cypate, ^64^Cu-DOTA-Y3-TATE-Lys-cypate
Agent category: | Peptide
Target: | Somatostatin receptor subtype-2 (SSTR-2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET), near-infrared (NIR) fluorescent imaging, optical fluorescent imaging
Source of signal/contrast: | ^64^Cu, cypate
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu + LS172)]

Somatostatin (SST) (somatotropin release-inhibiting hormone, somatotropin release-inhibiting factor) is a cyclic disulphide-containing peptide hormone of 14 amino acids (1). SST inhibits hormone secretion, cell proliferation, and promotes apoptosis through binding to specific cell-surface somatostatin receptors (SSTRs) (2). Five SSTR subtypes are identified in the central nervous system (CNS), gastrointestinal tract, and a variety of benign and malignant tumors (2). All subtypes of SSTRs belong to the family of G protein–coupled receptors, and exhibit high affinity to SST by recognizing the β-turn in the peptide sequence of SST including Phe7, Trp8, Lys9, and Thr10 (2). The structural difference between SSTRs generates specific pharmacological and physiological properties for each subtype, which allows targeting of SSTRs with subtype-specific SST analogs (1). For example, octreotide, a SST analog with a peptide sequence of eight amino acids (D-Phe-c(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(ol)), possesses a much higher affinity (~2 nM) binding to SSTR-2, -3, and -5 than binding to SSTR-1 and -4 (>1,000 nM). In addition to symptomatic treatment of tumors in clinic, these analogs are also labeled with a variety of probes for imaging (1).

^64^Cu-DOTA-Tyr^3^-c(Cys-Tyr-Trp-Lys-Thr-Cys)-Thr-Lys(cypate)-NH_2_ (^64^Cu-LS172) is a monomolecular multimodal imaging agent (MOMIA) for positron emission tomography (PET) and optical imaging (3). ^64^Cu-LS172 consists of three components: the STT analog Tyr3-octreotate (Y3-TATE) with an additional lysine at the N-terminal as a spacer linker, a complex of ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (^64^Cu-DOTA) attached at the C-terminal of Y3-TATE, and a cypate attached at the ε-amine group of the spacer lysine at the N-terminal of Y3-TATE. As a STT analog, TATE is produced by replacing the C-terminal threoninol in the octreotide with threonine, which substantially increases the binding affinity for SSTR-2 (1). ^64^Cu is a radionuclide belonged to IIB group with a half-life of 12.7 h. ^64^Cu has been a promising radionuclide in radiotherapy for effective short-range cell killing in tumors through β^-^ emission (578 keV; 38%). ^64^Cu is also a β^+^ emitter (653 keV) with modest positron yield (18%), which provides an adequate flux of annihilation photons for imaging its biodistribution by PET (4). Cypate (mw 625.34) is a carbocyanine derivative withstructure and optical properties very similar to indocyanine green dye (ICG). Cypate exhibits a high extinction coefficient (224,000 M^-1^cm^-1^) in the near-infrared (NIR) region (700–900 nm) (3, 6). The low light scattering and absorption of endogenous photoactive biomolecules in this region permit photons to penetrate several centimeters into tissues (7, 8). Two carboxyl groups in cypate can be conjugated with amines to generate peptide-based optical imaging agents (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + LS172)+AND+synthesis%0D%0A)]

The synthesis of ^64^Cu-LS172 was conducted in several steps (3). Y3-TATE was synthesized with a peptide synthesizer by standard automated Fmoc protocols. Rink amide resin was initially loaded with Fmoc amino acids, followed by automatic activation of the carboxyl group with a mixture of 1-hydroxybenzotriazole (HOBt) and o-(benzotriazol-1-yl)-N,N,N',N'-tetramethyluronium hexafluorophosphate (HBTU) and subsequent coupling with Fmoc-protected amino acid. LS172 was produced by attaching DOTA and cypate to Y3-TATE in situ. The carboxylic acid of tri-t-butyl-DOTA was coupled to the amine of the N-terminal phenylalanine, and the carboxylic acid of cypate was coupled to the ε-amino group of the C-terminal lysine. The overall yield of LS172 was found to be 96%. The radiolabling of LS172 was accomplished by mixing ^64^CuCl_2_ with LS172 in a buffer (pH 5.5) and incubated at 95ºC for 60 min. The produced ^64^Cu-LS172 had a radiochemical purity of ~80% and a final specific activity of 152 Ci/μg (332 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + LS172)+AND+%22in+vitro%22)]

The spectral and binding properties of LS172 were examined in vitro (3). Similar to cypate, LS172 exhibited broad excitation and emission bands with a narrow Stokes shift (23 nm). The relative quantum yield of LS172 (0.12) was the same as that of ICG. Complexation of LS172 with Cu^2+^ induced negligible reduction in the quantum yield. Because of the modifications in both C- and N-terminal, the affinity of LS172 binding to SSTR-2 increased ~10- and ~5-fold relative to cypate-Y3-TATE and Y3-TATE, respectively. But complexation with Cu^2+^ appeared not to affect the resultant affinity (11.5 nM for Cu-LS172 versus 2.03 nM for LS172). The internalization of LS172 and Cu-LS172 was evaluated with NIR fluorescence microscopy in A427-7 membranes (SSTR-2–positive) and HEK293 cells (STTR-2–negative). LS172 was weakly internalized at 25 nM. The internalization was inhibited by 5 μM Y3-TATE with an incubation time <60 min. Cu-LS172 appeared not to be internalized to any significant extent in cells. In comparison, cypate-Y3-TATE was strongly internalized in a time-dependent manner, and the internalization was completely blocked by 5 μM Y3-TATE.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + LS172) +AND++rodentia)]

The biochemical distribution of LS172 was examined in AR42J tumors in rats (n = 5) (3). ^64^Cu-LS172 (4 Ci/12 mmol (27 mg/12 mmol)) was injected intravenously in rats at 10–14 days after tumor implantation in the legs or after the tumors had grown ~1.5–2.0 g. In another group of tumor-implanted rats (n = 5), Y3-TATE (100μg/95 nmol) was also included as a competitive dose in addition to the radiolabeled LS172. The pharmacokinetic profile ^64^Cu-LS172 exhibited a rapid blood clearance of 0.228 ± 0.047% injected dose per gram (ID/g) (0.151 ± 0.027% ID/g) at 1 h after injection. Clearance of ^64^Cu-LS172 was predominately hepatic (16.824 ± 1.520% ID/g, 95.8 ± 7.12% ID/liver, 1 h) with relatively low kidney accumulation (1–2%). Accumulation of activity for ^64^Cu-LS172 in the SSTR-2–positive tissues of adrenal, pituitary, pancreas, and tumor were relatively low (≤1% ID/g). ^64^Cu-LS172 accumulation in tumors decreased in the presence of Y3-TATE, but the observed decrease in other SSTR-2–positive organs was not significant.

The NIR fluorescence imaging of LS172 was performed in tumor-bearing NCR nu/nu mice (n = 6) (3). After inoculation with lung adenocarcinoma cell line A427-7 in the right and left flanks of each mouse, tumors were allowed to grow to 5–10 mm maximum diameter before imaging. Three mice were injected with 2 nmol LS172, and two other mice were injected with 2 nmol LS172 and a competitive dose of 95 nmol Y3-TATE. NIR fluorescence images were collected at 1, 4, 8, and 24 h after injection. No significant accumulation of LS172 was found in tumors compared to normal tissue at different time points. The competitive inhibition with Y3-TATE did not significantly alter the tumor/muscle uptake ratio. After 24 h, the mice were euthanized, and tissues were harvested for ex vivo fluorescence biodistribution imaging. In addition to the liver and kidneys, LS172 accumulated in the spleen and accounted for 35% of the fluorescence intensity relative to that in the liver. LS172 accumulation in mouse kidney was somewhat higher than that of the radiolabeled analogs in rat kidneys, possibly indicating the reduction of overall charge on the DOTA upon chelation with a metal ion. The uptake and clearance profiles of LS172 in tumor-bearing A427-7 mice were similar to those of ^64^Cu-LS172 in tumor-bearing AR427 rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + LS172) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + LS172) +AND+human)]

No publication is currently available.

### NIH Support

CA 100972, EB 1430, CA 123537, CA 64475

## References

1 Breeman W.A., Kwekkeboom D.J., de Blois E., de Jong M., Visser T.J., Krenning E.P. (2007). Radiolabelled regulatory peptides for imaging and therapy. Anticancer Agents Med Chem.
2 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
3 Edwards W.B., Xu B., Akers W., Cheney P.P., Liang K., Rogers B.E., Anderson C.J., Achilefu S. (2008). Agonist-antagonist dilemma in molecular imaging: evaluation of a monomolecular multimodal imaging agent for the somatostatin receptor. Bioconjug Chem.
4 Cutler P.D., Schwarz S.W., Anderson C.J., Connett J.M., Welch M.J., Philpott G.W., Siegel B.A. (1995). Dosimetry of copper-64-labeled monoclonal antibody 1A3 as determined by PET imaging of the torso. J Nucl Med.
5 Sun X., Anderson C.J. (2004). Production and applications of copper-64 radiopharmaceuticals. Methods Enzymol.
6 Achilefu S., Dorshow R.B., Bugaj J.E., Rajagopalan R. (2000). Novel receptor-targeted fluorescent contrast agents for in vivo tumor imaging. Invest Radiol.
7 Mahmood U., Weissleder R. (2003). Near-infrared optical imaging of proteases in cancer. Mol Cancer Ther.
8 Ye Y., Bloch S., Xu B., Achilefu S. (2008). Novel near-infrared fluorescent integrin-targeted DFO analogue. Bioconjug Chem.
9 Zhang Z., Achilefu S. (2005). Spectral properties of pro-multimodal imaging agents derived from a NIR dye and a metal chelator. Photochem Photobiol.